# [^18^F]Fluoromethyl-D-tyrosine

Chemical name: | [^18^F]Fluoromethyl- D-tyrosine
Abbreviated name: | D-[^18^F]FMT
Synonym:
Agent Category: | Compound
Target: | L-amino acid transporter 1
Target Category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+fluoromethyl+D+tyrosine)]

Cancerous tumors are formed by characteristically high levels of proliferating cells that have a constant high requirement for basic building blocks such as carbohydrates, nucleotides, and amino acids (AA) to maintain a suitable metabolic rate and to continue the synthesis of macromolecules such as DNA and proteins to sustain their phenotype (1). Because of the high carbohydrate demand of tumor cells, (^18^F)fluorodeoxy-glucose ((^18^F)FDG), which is not metabolized by the cells and as a consequence accumulates in neoplastic tumors, was developed to screen for cancers using positron emission tomography (PET) imaging. Although shown to be suitable for the detection of certain cancers (2), the main limitation of using (^18^F)FDG to detect tumors is that it tends to accumulate in some normal tissues (e.g., brain and heart) and inflamed tissues (3-5). Therefore, several ^11^C- and ^18^F-labeled AAs and their analogs, including L- and D-methyl-^11^C-methionine (L- and D-(^11^C)MET) and L- and D-O-(^18^F)fluoromethyl-tyrosine (L- and D-(^18^F)FMT), were developed as an alternative and have been evaluated for the uptake by and PET imaging of normal and tumor tissues (6, 7).

Radiolabeled L-isomers of AAs behave like the naturally occurring compounds in a biological system, can be used for protein synthesis, are easily metabolized by mammalian cells, and have been shown to accumulate in non-target tissue in addition to tumors (8). In contrast, the D-isomers are unnatural and, compared with the L-isomers, ^14^C-labeled D-amino acids have been shown to have a higher tumor accumulation (9-12). Although different AA transport systems are involved in the uptake of AAs, the AAs are transported primarily by the L AA transport systems (designated as LAT1 and LAT2), which are not sodium-dependent and can transport both the L- and D-isomers (7, 13), including those containing a branched chain or an aromatic moiety (14). Also, the LAT1 was reported to be expressed in the brain, spleen, placenta, and the testis (15) and was reported to be overexpressed in malignant tumors (16, 17). Tsukada et al. reported the tumor/blood uptake of the D-isomers of (^18^F)FMT, (^18^F)fluoroethyl-tyrosine, and (^18^F)fluoropropyl-tyrosine in tumor-bearing mice was 181%, 137%, and 101%, respectively, compared with their L homologs, indicating that the D-isomers could be potential PET imaging agents (13). In another study, D-(^18^F)FMT was suggested to be a better PET tracer than the L- and D-isomers of (^11^C)MET because it showed lower accumulation in various normal organs and, compared with (^18^F)FDG, did not accumulate in inflamed tissue (7). Urakami et al. studied the uptake of L- and D-(^18^F)FMT in cultured cells under in vitro conditions and evaluated the use of these radiolabeled compounds for the imaging of abdominal and brain tumors in rats and mice, respectively (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMT+synthesis)]

The L- and D-isomers of tyrosine were reacted with (^18^F)fluoromethyl bromide to generate (^18^F)FMT as described elsewhere (7, 13). Purity of the two enantiomers was determined with high-performance liquid chromatography using a CHIOBIOTIC T column with ethanol:water (1:1) as the eluent. (^18^F)FDG was produced as detailed by Oberdorfer et al. (19). The specific activities of D-(^18^F)FMT, L-(^18^F)FMT, and (^18^F)FDG were 115 ± 10, 126 ± 12, and 144 ± 21 GBq/μmol, respectively (3.10 ± 0.27, 3.40 ± 0.32, and 3.89 ± 0.56 Ci/μmol, respectively) (18). The radiochemical purities of D-(^18^F)FMT, L-(^18^F)FMT, and (^18^F)FDG were 99.6 ± 0.4%, 99.8 ± 0.3%, and 100.0 ± 0.0%, respectively (18). The average time of radiochemical synthesis and the yield of these labeled compounds were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMT+in+vitro)]

Urakami et al. studied the uptake of d-(18F)FMT and l-(18F)FMT in rat C6 glioma and HeLa cells at select time points for up to 30 min after exposure to the radiochemicals (18). Both cell lines were reported to show a higher uptake of the l-isomer, and the uptake was not saturated even at 60 min. The release of both labeled isomers was studied using HeLa cells loaded with the l- and d-isomers, respectively, in AA-free medium and in presence or absence of excess l-leucine (100 μM) (18). Presence of l-leucine was reported to accelerate the release of both labeled isomers from the loaded HeLa cells. The uptake and release study indicated that the transport of the labeled d-isomer was lower than the transport of the l-isomer under in vitro conditions. In another study, the uptake of both labeled isomers in C6 glioma cells was reported to be inhibited by the presence of excess (1 mM) l-isomers of methionine, phenylalanine, and tyrosine. Uptake of the two labeled isomers was also inhibited by 2-aminobicyclo-(2,2,1)-heptane-2-carboxylic acid, a selective inhibitor of the l AA transport system, but no inhibition was observed with l-glycine. These results indicated that both the labeled isomers were transported by the l AA transport system (18). This observation was confirmed with a reverse-transcriptase polymerase chain reaction analysis of the C6 glioma and HeLa cells, and it was observed that only the LAT1 mRNA was expressed in both the cell lines.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMT+rodentia)]

Urakami et al. evaluated the use of D-(^18^F)FMT, L-(^18^F)FMT, and (^18^F)FDG, respectively, for PET imaging in normal tissue (left leg) and HeLa cell xenograft tumors (right leg) in mice (n > 3 animals for each radiocompound) (18). The standard uptake values (SUV) for D-(^18^F)FMT and L-(^18^F)FMT in the tumor tissue were 1.33 and 1.642, respectively, but these values were 0.488 and 0.874, respectively, in the normal tissue. Therefore, among these labeled compounds, D-(^18^F)FMT was reported to show a more clear difference between the normal tissue and tumor tissue. Under the same experimental conditions, (^18^F)FDG was reported to have a lower accumulation in the tumor compared with either (^18^F)FMT isomer, and an uptake of the labeled carbohydrate derivative was also observed in the normal brain and heart of the animals.

Another study performed to image C6 glioma tumors in mouse brain (n = 5 animals per labeled compound) also showed that D-(^18^F)FMT was a superior PET imaging agent compared with either L-(^18^F)FMT or (^18^F)FDG (18).

Tsukada et al. compared the use of D-(^18^F)FMT to the use of O-^11^C-methyl-D-tyrosine (D-(^11^C)CMT) and to D- and L-(^11^C)MET for the PET imaging of HeLa tumors in mice (n = 5 animals per labeled AA) (7). Although the tumor SUV levels of D-isomers of (^11^C)MET, (^11^C)CMT, and (^18^F)FMT were 261%, 72%, and 95%, respectively, of the corresponding L-isomer of the AAs at 60 min after administration, the tumor/blood ratios of the D-isomers were reported to be 130%, 140%, and 182%, respectively, of the L-isomers. Also, the D-isomers of the various labeled AAs had a much lower uptake in the abdominal organs compared with L-isomers of AAs. The investigators also compared the uptake of D- and L-(^11^C)MET, D-(^11^C)CMT, and D-(^18^F)FMT to (^18^F)FDG for the visualization of turpentine-induced inflammatory tissue in these animals (n = 5 mice per labeled AA) (7). Among these labeled compounds, only (^18^F)FDG was reported to show a high accumulation in the inflamed tissue. From these studies the investigators concluded that the D-isomers of (^11^C)CMT and (^18^F)FMT were probably superior to L- and D-(^11^C)MET for tumor imaging using PET.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMT+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMT+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FMT+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

## References

1 Ganapathy V., Thangaraju M., Prasad P.D. (2009). Nutrient transporters in cancer: relevance to Warburg hypothesis and beyond. Pharmacol Ther.
2 Yamazaki Y., Saitoh M., Notani K., Tei K., Totsuka Y., Takinami S., Kanegae K., Inubushi M., Tamaki N., Kitagawa Y. (2008). Assessment of cervical lymph node metastases using FDG-PET in patients with head and neck cancer. Ann Nucl Med.
3 Miyamoto J., Tatsuzawa K., Owada K., Kawabe T., Sasajima H., Mineura K. (2008). Usefulness and limitations of fluorine-18-fluorodeoxyglucose positron emission tomography for the detection of malignancy of orbital tumors. Neurol Med Chir (Tokyo).
4 Suzuki H., Hasegawa Y., Terada A., Ogawa T., Hyodo I., Suzuki M., Nakashima T., Tamaki T., Nishio M. (2008). Limitations of FDG-PET and FDG-PET with computed tomography for detecting synchronous cancer in pharyngeal cancer. Arch Otolaryngol Head Neck Surg.
5 Terauchi T., Murano T., Daisaki H., Kanou D., Shoda H., Kakinuma R., Hamashima C., Moriyama N., Kakizoe T. (2008). Evaluation of whole-body cancer screening using 18F-2-deoxy-2-fluoro-D-glucose positron emission tomography: a preliminary report. Ann Nucl Med.
6 Ishiwata K., Kawamura K., Wang W.F., Furumoto S., Kubota K., Pascali C., Bogni A., Iwata R. (2004). Evaluation of O-[11C]methyl-L-tyrosine and O-[18F]fluoromethyl-L-tyrosine as tumor imaging tracers by PET. Nucl Med Biol.
7 Tsukada H., Sato K., Fukumoto D., Nishiyama S., Harada N., Kakiuchi T. (2006). Evaluation of D-isomers of O-11C-methyl tyrosine and O-18F-fluoromethyl tyrosine as tumor-imaging agents in tumor-bearing mice: comparison with L- and D-11C-methionine. J Nucl Med.
8 Bauwens M., Keyaerts M., Lahoutte T., Kersemans K., Caveliers V., Bossuyt A., Mertens J. (2007). Intra-individual comparison of the human biodistribution and dosimetry of the D and L isomers of 2-[123I]iodo-phenylalanine. Nucl Med Commun.
9 Bauwens M., Lahoutte T., Kersemans K., Gallez C., Bossuyt A., Mertens J. (2006). Comparison of the uptake of [123/125I]-2-iodo-D-tyrosine and [123/125I]-2-iodo-L-tyrosine in R1M rhabdomyosarcoma cells in vitro and in R1M tumor-bearing Wag/Rij rats in vivo. Nucl Med Biol.
10 Kersemans V., Cornelissen B., Bacher K., Kersemans K., Thierens H., Dierckx R.A., De Spiegeleer B., Slegers G., Mertens J. (2005). In vivo evaluation and dosimetry of 123I-2-iodo-D-phenylalanine, a new potential tumor-specific tracer for SPECT, in an R1M rhabdomyosarcoma athymic mouse model. J Nucl Med.
11 Kersemans V., Cornelissen B., Kersemans K., Bauwens M., Achten E., Dierckx R.A., Mertens J., Slegers G. (2005). In vivo characterization of 123/125I-2-iodo-L-phenylalanine in an R1M rhabdomyosarcoma athymic mouse model as a potential tumor tracer for SPECT. J Nucl Med.
12 Foulon C.F., Reist C.J., Bigner D.D., Zalutsky M.R. (2000). Radioiodination via D-amino acid peptide enhances cellular retention and tumor xenograft targeting of an internalizing anti-epidermal growth factor receptor variant III monoclonal antibody. Cancer Res.
13 Tsukada H., Sato K., Fukumoto D., Kakiuchi T. (2006). Evaluation of D-isomers of O-18F-fluoromethyl, O-18F-fluoroethyl and O-18F-fluoropropyl tyrosine as tumour imaging agents in mice. Eur J Nucl Med Mol Imaging.
14 Kanai Y., Endou H. (2001). Heterodimeric amino acid transporters: molecular biology and pathological and pharmacological relevance. Curr Drug Metab.
15 Prasad P.D., Wang H., Huang W., Kekuda R., Rajan D.P., Leibach F.H., Ganapathy V. (1999). Human LAT1, a subunit of system L amino acid transporter: molecular cloning and transport function. Biochem Biophys Res Commun.
16 Kim D.K., Kim I.J., Hwang S., Kook J.H., Lee M.C., Shin B.A., Bae C.S., Yoon J.H., Ahn S.G., Kim S.A., Kanai Y., Endou H., Kim J.K. (2004). System L-amino acid transporters are differently expressed in rat astrocyte and C6 glioma cells. Neurosci Res.
17 Yanagida O., Kanai Y., Chairoungdua A., Kim D.K., Segawa H., Nii T., Cha S.H., Matsuo H., Fukushima J., Fukasawa Y., Tani Y., Taketani Y., Uchino H., Kim J.Y., Inatomi J., Okayasu I., Miyamoto K., Takeda E., Goya T., Endou H. (2001). Human L-type amino acid transporter 1 (LAT1): characterization of function and expression in tumor cell lines. Biochim Biophys Acta.
18 Urakami T., Sakai K., Asai T., Fukumoto D., Tsukada H., Oku N. (2009). Evaluation of O-[(18)F]fluoromethyl-d-tyrosine as a radiotracer for tumor imaging with positron emission tomography. Nucl Med Biol.
19 Oberdorfer F., Hull W.E., Traving B.C., Maier-Borst W. (1986). Synthesis and purification of 2-deoxy-2-[18F]fluoro-D-glucose and 2-deoxy-2-[18F]fluoro-D-mannose: characterization of products by 1H- and 19F-NMR spectroscopy. Int J Rad Appl Instrum [A].